# ^99m^Tc-Glucosamino-Asp-cyclo(Arg-Gly-Asp-D-Phe-Lys)

Chemical name: | ^99m^Tc-Glucosamino-Asp-cyclo(Arg-Gly-Asp-D-Phe-Lys)
Abbreviated name: | Glucosamino ^99m^Tc-D-c(RGDfK)
Synonym:
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | SPECT, gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+glucosamino+RGD)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (inhibition concentration (IC_50_), 7–40 nM) but not to integrins α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM). Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). Jung et al. (13) reported the development of glucosamino ^99m^Tc-D-c(RGDfK) that contains N-D-glucosamine as a sugar moiety for imaging α_v_β_3_ receptors during tumor angiogenesis.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+glucosamino+RGD+synthesis)]

Jung et al. (13) synthesized glucosamino ^99m^Tc-D-c(RGDfK) by reacting glucosamino [N-α-bis(hydroxycarbonylmethyl)-G]-D-c(RGDfK) with [^99m^Tc(H_2_O)_3_(CO)_3_]^+^ in a mixture of methanol and water at 65°C for 30 min, followed by purification with high-performance liquid chromatography. Radiochemical yield and specific activity were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+glucosamino+RGD+in+vitro)]

Jung et al. (13) performed in vitro binding studies of glucosamino ^99m^Tc-D-c(RGDfK) in cultured human umbilical endothelial cells (HUVEC), RR1022 fibrosarcoma cells, and Lewis lung carcinoma (LLC) cells. Excess c(RGDyV) (10 μM) inhibited cellular uptake of glucosamino ^99m^Tc-D-c(RGDfK) by 80% in HUVEC (P < 0.0001) and by 44% in RR1022 cells (P < 0.05), whereas no inhibition was observed in LLC cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+glucosamino+RGD+rodentia)]

Jung et al. (13) performed biodistribution studies of glucosamino ^99m^Tc-D-c(RGDfK) in nude mice bearing RR1022 or LLC tumors. The initial tracer accumulation in the RR1022 tumors expressing the α_v_β_3_ integrin was 1.03 ± 0.21% injected dose (ID)/g at 1 h and decreased to 0.85 ± 0.05% ID/g at 4 h. At 1 h, the highest radioactive concentration was found in the kidney (3.33% ID/g), followed by the liver (2.99% ID/g) and stomach (1.77% ID/g). Blood levels were 0.50% ID/g at 1 h and 0.19% ID/g at 4 h. The tracer accumulation in the LLC tumor negative for the α_v_β_3_ receptor was 1.18 ± 0.26% ID/g at 1 h and decreased to 0.89 ± 0.28% ID/g at 4 h. Hence, endothelial cells may have mainly contributed to the LLC tumor (negative for α_v_β_3_ integrin) accumulation. Blood levels were 1.19% ID/g at 1 h and 0.19% ID/g at 4 h. The radioactivity levels in other organs were similar to those of mice bearing RR1022 tumors. Pretreatment with excess c(RGDyV) (9 mg/kg) 10 min before glucosamino ^99m^Tc-D-c(RGDfK) reduced accumulation by 76.5% in RR1022 tumors and by 70.2% in LLC tumors. Single-photon emission computed tomography (SPECT) gamma planar imaging was performed in mice bearing RR1022 and LLC tumors 4 h after injection of glucosamino ^99m^Tc-D-c(RGDfK). Both tumors were clearly visualized with a tumor/thigh ratio of 10.1 ± 2.2 for RR1022 tumors and 9.8 ± 4.9 for LLC tumors. Pretreatment with excess c(RGDyV) significantly reduced tumor contrast in RR1022 tumors (P < 0.01). No pretreatment SPECT experiment was performed in mice bearing LLC tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+glucosamino+RGD+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+glucosamino+RGD+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+glucosamino+RGD+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Jung K.H., Lee K.H., Paik J.Y., Ko B.H., Bae J.S., Lee B.C., Sung H.J., Kim D.H., Choe Y.S., Chi D.Y. (2006). Favorable biokinetic and tumor-targeting properties of 99mTc-labeled glucosamino RGD and effect of paclitaxel therapy. J Nucl Med.